# ^99m^Tc-Labeled S-benzoylmercaptoacetyl triglycine D-glucose

Chemical name: | ^99m^Tc-Labeled S-benzoylmercaptoacetyl triglycine D-glucose
Abbreviated name: | [^99m^Tc]SBz-MAG_3_-Gl
Synonym: | [^99m^Tc]MAG_3_-Gl
Agent Category: | Compound
Target: | Lectins
Target Category: | Proteins
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure of [^99m^Tc]SBz-MAG_3_-Gl. Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=lectins&cmd=DetailsSearch)]

Lectins are proteins that bind carbohydrates reversibly and are present on the membrane surface of all prokaryotic and eukaryotic cells. It is known that the carbohydrate–lectin interactions result in the initiation of a fight against or the development of a variety of conditions such as cancer metastases (1), pathological inflammation (2), and microbial infections (3). Several clinical trials (http://clinicaltrials.gov/ct2/results?term=lectins) approved by the United States Food and Drug Administration are under way to evaluate the use of lectins to treat a variety of infections and cancerous tumors. Because of their role in the modulation of diverse physiological processes and diseases, investigators are increasingly interested in studying lectins for the development (4) and delivery of therapeutic drugs in humans (5). Although lectin glycoarrays have been used to profile different glycoproteins (6), no agents are presently available to investigate the function of the lectin-carbohydrate complexes under in vivo conditions. In an effort to develop imaging agents for the in vivo study of lectins, de Barros et al. (7) synthesized glucose (Gl), N-acetylglucosamine (NG), and galactose (Ga) respectively conjugated to S-benzoylmercaptoacetyl triglycine (SBz-MAG_3_) and labeled these compounds with ^99m^Tc to obtain [^99m^Tc]SBz-MAG_3_-Gl (or [^99m^Tc]MAG_3_-Gl), [^99m^Tc]SBz-MAG_3_-NG (or [^99m^Tc]MAG_3_-NG), and [^99m^Tc]SBz-MAG_3_-Ga (or [^99m^Tc]MAG_3_-Ga). The biodistribution of these radiolabeled carbohydrates was then studied in normal and Ehrlich tumor-bearing Swiss mice (7, 8). This chapter describes the results obtained with [^99m^Tc]SBz-MAG_3_-Gl. Results obtained with [^99m^Tc]SBz-MAG_3_-NG (9) and [^99m^Tc]SBz-MAG_3_-Ga (10) are presented in separate chapters in MICAD (www.micad.nih.gov).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S%20benzoylmercaptoacetyl%20triglycine%20D%20glucose%20synthesis&cmd=DetailsSearch)]

The synthesis of [^99m^Tc]SBzMAG_3_-Gl was described by de Barros et al. (7). The radiochemical purity of the tracer was reported to be >90%. The radiochemical yield, specific activity, and stability of [^99m^Tc]SBzMAG_3_-Gl were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S%20benzoylmercaptoacetyl%20triglycine%20D%20glucose%20in%20Vitro%20studies&cmd=DetailsSearch)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S%20benzoylmercaptoacetyl%20triglycine%20D%20glucose%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]SBz-MAG_3_-Gl was studied in normal Swiss mice (7). The animals (n = 5 mice per time point) were injected with the radiochemical, and the mice were euthanized at various time points from 5 to 60 min post-injection (p.i.) to collect all major organs and to determine the accumulated radioactivity. At 5 min p.i., the bladder had maximum uptake of the label (41.17 ± 5.40% injected dose per gram tissue (% ID/g)), followed by the kidneys (22.97 ± 3.91% ID/g), liver (8.77 ± 1.22% ID/g), blood (3.28 ± 0.21% ID/g), and lungs (2.11 ± 0.27% ID/g). At 60 min p.i., the bladder had the highest amount of radioactivity (94.24 ± 4.19% ID/g), followed by liver (1.82 ± 0.15% ID/g), kidneys (1.24 ± 0.16% ID/g), lungs (0.63 ± 0.08% ID/g), and blood (0.57 ± 0.06% ID/g). This study indicated that radioactivity either as [^99m^Tc]SBz-MAG_3_-Gl or a metabolite was excreted primarily through the urinary route. The radioactivity uptake pattern with [^99m^Tc]SBz-MAG_3_-Gl was similar to that observed with [^99m^Tc]SBz-MAG_3_-NG (9) and [^99m^Tc]SBz-MAG_3_-Ga (10). However, accumulation of [^99m^Tc]SBz-MAG_3_-Ga was significantly (P < 0.05) higher in the liver than accumulation of either [^99m^Tc]SBz-MAG_3_-Gl (8.77 ± 1.22% ID/g at 5 min and 1.82 ± 0.15% ID/g at 60 min p.i.) or [^99m^Tc]SBz-MAG_3_-NG (9.58 ± 0.81% ID/g at 5 min and 1.88 ± 0.44% ID/g at 60 min p.i.).

In another study, the use of [^99m^Tc]SBz-MAG_3_-Gl for the detection of Ehrlich tumors in mice was evaluated by de Barros et al. (8). The animals were injected with the tracer and euthanized at intervals ranging from 5 to 480 min p.i. (n = 5 mice per time point) to determine the amount of accumulated radioactivity in the various organs. The biodistribution pattern of the label in the various organs was as described above. The tumor/muscle ratio was 1.96 ± 0.34 at 5 min p.i. and increased to 5.03 ± 0.98 at 480 min p.i. During the same period, the tumor/blood ratio changed from 0.55 ± 0.21 at 5 min p.i. to 2.42 ± 0.50 at 480 min p.i. No blocking studies were reported.

From these studies, the investigators concluded that, although ^99m^Tc-MAG_3_-Gl appeared to be a suitable agent for the detection of tumors in rodents, more studies are necessary to confirm this observation (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S-benzoylmercaptoacetyl%20triglycine%20glucose%20non%20primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S-benzoylmercaptoacetyl%20triglycine%20glucose%20non%20human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%20S-benzoylmercaptoacetyl%20triglycine%20glucose%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Makrilia N., Kollias A., Manolopoulos L., Syrigos K. (2009). Cell adhesion molecules: role and clinical significance in cancer. Cancer Invest.
2 Yang R.Y., Rabinovich G.A., Liu F.T. (2008). Galectins: structure, function and therapeutic potential. Expert Rev Mol Med.
3 Haagsman H.P., Hogenkamp A., van Eijk M., Veldhuizen E.J. (2008). Surfactant collectins and innate immunity. Neonatology.
4 Ernst B., Magnani J.L. (2009). From carbohydrate leads to glycomimetic drugs. Nat Rev Drug Discov.
5 Darbre T., Reymond J.L. (2008). Glycopeptide dendrimers for biomedical applications. Curr Top Med Chem.
6 Zhao J., Patwa T.H., Qiu W., Shedden K., Hinderer R., Misek D.E., Anderson M.A., Simeone D.M., Lubman D.M. (2007). Glycoprotein microarrays with multi-lectin detection: unique lectin binding patterns as a tool for classifying normal, chronic pancreatitis and pancreatic cancer sera. J Proteome Res.
7 de Barros, A.L., V.N. Cardoso, L.D. Mota, and R.J. Alves, Synthesis and biodistribution studies of carbohydrate derivatives radiolabeled with technetium-99m. Bioorg Med Chem Lett, 2009
8 de Barros A.L., Cardoso V.N., Mota L.G., Leite E.A., Oliveira M.C., Alves R.J. (2009). Synthesis and biological evaluation of technetium-labeled D-glucose-MAG3 derivative as agent for tumor diagnosis. Bioorg Med Chem Lett.
9 Chopra, A., 99mTc-Labeled S-benzoylmercaptoacetyl triglycine N-acetylglucosamine. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
10 Chopra, A., 99mTc-Labeled S-benzoylmercaptoacetyl triglycine D-galactose. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.